# [^18^F]-N-(2-Chloro-6-methylphenyl)-2-(6-(4-(2-fluoroethyl)piperazin-1-yl)-2-methylpyrimidin-4-ylamino)thiazole-5-carboxamide

Chemical name: | [^18^F]-N-(2-Chloro-6-methylphenyl)-2-(6-(4-(2-fluoroethyl)piperazin-1-yl)-2-methylpyrimidin-4-ylamino)thiazole-5-carboxamide
Abbreviated name: | [^18^F]SKI-249380
Synonym:
Agent Category: | Compound
Target: | Tyrosine kinases
Target Category: | Competitive enzyme inhibitor
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+Dasatinib)]

Imatinib (4-[(4-methyl-1-piperazinyl)methyl]-N-[4-methyl-3-[[4-(3-pyridyl)-2-pyrimidinyl]amino]phenyl]benzamide) is a tyrosine kinase (TK) inhibitor used for the treatment of chronic myeloid leukemia (CML) attributed to the Philadelphia chromosome (Ph+) (1). This chromosomal abnormality develops after a genetic translocation between chromosome 9 and chromosome 22, which leads to the expression of a constitutively activated Bcr-Abl TK that is no longer under normal regulation. This drug is also used for the treatment of gastrointestinal stromal tumors (GIST) that are caused by mutations in the closely related Kit or platelet-derived growth factor (PDGF) TKs (2). In addition, imatinib has been shown to be an effective treatment against a variety of other conditions that are characterized by the expression of Abl or c-Kit TKs (3). Although imatinib is a useful chemotherapeutic agent for the treatment of CML and GIST, patients undergoing therapy for these conditions often develop resistance to the drug as a result of secondary mutations in the TKs (4). Dasatinib is a dual inhibitor of Src/Abl and c-Kit that was recently approved for treatment of imatinib-refractory CML and Ph+ acute lymphoblastic leukemia (ALL) (5, 6). A [^18^F]fluorine derivative of dasatinib ([^18^F]-N-(2-chloro-6-methylphenyl)-2-(6-(4-(2-fluoroethyl)piperazin-1-yl)-2-methylpyrimidin-4-ylamino)thiazole-5-carboxamide ([^18^F]SKI-249380)) was synthesized to probe the role of Abl, Src, and c-Kit in tumor malignancies with positron emission tomography (PET) imaging in small animals (7).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+Dasatinib+synthesis)]

[^18^F]-1-Bromo-2-fluoroethane was reacted with N-(2-chloro-6-methylphenyl)-2-(2-methyl-6-(piperazin-1-yl)pyrimidin-4-ylamino)thiazole-5-carboxamide for 40 min at 120ºC. The radiochemical purity of the labeled product as determined with high-performance liquid chromatography was >99%. The total synthesis time was 2 h from the end of bombardment. Specific activity of the radiochemical was reported to be 4.1–271.9 GBq/µmol (0.11–7.35 Ci/µmol, n = 11) at the end of bombardment. The decay-corrected radiochemical yield was 25.1 ± 5.8% from [^18^F]-1-bromo-2-fluoroethane.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+Dasatinib+in+vitro)]

SKI-249380 exhibited a binding profile to a panel of 21 kinases similar to that of dasatinib. Abl, Src, and Kit were inhibited by >97% at 10 nM with IC_50_ values of ~2 nM (7).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+Dasatinib+rodentia)]

Veach et al. (7) performed a preliminary study in nude mice (n = 3) bearing subcutaneous K562 (CML) tumor xenografts. PET was used to image [^18^F]SKI-249380 (13.9 MBq (0.375 mCi)) 60–90 min after injection. [^18^F]SKI-249380 radioactivity accumulated mainly in the liver, intestines, kidneys, and urinary bladder. The tumor was clearly visualized, and radioactivity accumulation was determined to be 1.1% of the injected dose. No accumulation was observed in the bones. No blocking experiment or correlation of Bcr-Abl tumor expression with tumor uptake was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+Dasatinib+(Dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+Dasatinib+(primate%20not%20human))]

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+Dasatinib+human)]

No publication is currently available.

## NIH Support

CA08748, CA86438, CA83084

## References

1 Moen M.D., McKeage K., Plosker G.L., Siddiqui M.A. (2007). Imatinib: a review of its use in chronic myeloid leukaemia. Drugs.
2 Rubin B.P., Heinrich M.C., Corless C.L. (2007). Gastrointestinal stromal tumour. Lancet.
3 Kil K.E., Ding Y.S., Lin K.S., Alexoff D., Kim S.W., Shea C., Xu Y., Muench L., Fowler J.S. (2007). Synthesis and positron emission tomography studies of carbon-11-labeled imatinib (Gleevec). Nucl Med Biol.
4 Deininger M., Buchdunger E., Druker B.J. (2005). The development of imatinib as a therapeutic agent for chronic myeloid leukemia. Blood.
5 Lombardo L.J., Lee F.Y., Chen P., Norris D., Barrish J.C., Behnia K., Castaneda S., Cornelius L.A., Das J., Doweyko A.M., Fairchild C., Hunt J.T., Inigo I., Johnston K., Kamath A., Kan D., Klei H., Marathe P., Pang S., Peterson R., Pitt S., Schieven G.L., Schmidt R.J., Tokarski J., Wen M.L., Wityak J., Borzilleri R.M. (2004). Discovery of N-(2-chloro-6-methyl- phenyl)-2-(6-(4-(2-hydroxyethyl)- piperazin-1-yl)-2-methylpyrimidin-4- ylamino)thiazole-5-carboxamide (BMS-354825), a dual Src/Abl kinase inhibitor with potent antitumor activity in preclinical assays. J Med Chem.
6 Steinberg M. (2007). Dasatinib: a tyrosine kinase inhibitor for the treatment of chronic myelogenous leukemia and philadelphia chromosome-positive acute lymphoblastic leukemia. Clin Ther.
7 Veach D.R., Namavari M., Pillarsetty N., Santos E.B., Beresten-Kochetkov T., Lambek C., Punzalan B.J., Antczak C., Smith-Jones P.M., Djaballah H., Clarkson B., Larson S.M. (2007). Synthesis and biological evaluation of a fluorine-18 derivative of dasatinib. J Med Chem.